# ^68^Ga-1,4,7-Triazacyclononane-1,4,7-triacetic acid-polyethylene glycol-single-chain Cys-tagged vascular endothelial growth factor-121

Chemical name: | ^68^Ga-1,4,7-Triazacyclononane-1,4,7-triacetic acid-polyethylene glycol-single-chain Cys-tagged vascular endothelial growth factor-121
Abbreviated name: | ^68^Ga-NOTA-PEG-scVEGF
Synonym:
Agent category: | Polypeptide
Target: | Vascular endothelial growth factor receptor-2 (VEGFR-2)
Target category: | Receptor
Method of detection: | Positron emission tomography (PET)
Source of signal: | ^68^Ga
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&val=71051581), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?val=NM_001025368.1) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=Graphics&list_uids=7422) for more information about VEGF.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=scVEGF)]

Vascular endothelial growth factor (VEGF) consists of at least six isoforms with various numbers of amino acids (121, 145, 165, 183, 189, and 206 amino acids) produced through alternative splicing (1). VEGF_121_, VEGF_165_, and VEGF_189_ are the forms secreted by most cell types and are active as homodimers linked by disulfide bonds. VEGF_121_ does not bind to heparin like the other VEGF species do (2). VEGF is a potent angiogenic factor that induces proliferation, sprouting, migration, and tube formation of endothelial cells. There are three high-affinity tyrosine kinase VEGF receptors (VEGFRs) on endothelial cells (VEGFR-1, Flt-1; VEGFR-2, KDR/Flt-1; and VEGFR-3, Flt-4). Several types of non-endothelial cells, such as hematopoietic stem cells, melanoma cells, monocytes, osteoblasts, and pancreatic β cells, also express VEGFRs (1).

VEGFRs have been found to be overexpressed in various tumor cells and tumor-associated endothelial cells but are not detectable in quiescent endothelial cells (3). Inhibition of VEGFR function has been shown to inhibit pathological angiogenesis as well as tumor growth and metastasis (4, 5). Radiolabeled VEGF has been developed as a tracer for imaging solid tumors and angiogenesis in humans (6-8). A 15-amino-acid fusion tag (Cys-tag) was developed for site-specific conjugation via the free sulfhydryl group of Cys. Backer et al. (9) prepared a Cys-tagged vector of VEGF_121_ by cloning two single-chain 3–112 amino acid fragments of VEGF_121_ joining head-to-tail to express as scVEGF, which was labeled as ^64^Cu-1,4,7,10-tetraazacyclododecane-1,4,7,10-tetraacetic acid (DOTA)-polyethylene glycol (PEG)-scVEGF (^64^Cu-DOTA-PEG-scVEGF), ^99m^Tc-hydrazinonicotinic acid (HYNIC)-scVEGF (^99m^Tc-HYNIC-scVEGF), and Cy5.5-scVEGF for imaging VEGFR expression to study tumor angiogenesis. In this chapter, ^68^Ga-1,4,7-Triazacyclononane-1,4,7-triacetic acid-PEG-scVEGF (^68^Ga-NOTA-PEG-scVEGF) is being developed for positron emission tomography (PET) imaging of VEGFR-2 in tumor vasculature (10).

### Related Resource Links:

- Chapters in MICAD (VEGFR (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=books&Cmd=DetailsSearch&Term=VEGFR+AND+micad%5Bbook%5D))
- Gene information in NCBI (VEGFR (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=gene&Cmd=DetailsSearch&Term=3791))
- Articles in Online Mendelian Inheritance in Man (OMIM) (VEGFR (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=omim&Cmd=DetailsSearch&Term=VEGFR))
- Clinical trials (VEGFR (http://www.clinicaltrials.gov/ct2/results?term=VEGFR))
- FDA Drug information (VEGFR (http://google2.fda.gov/search?q=VEGFR&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=12&y=7))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=scVEGF+synthesis)]

Backer et al. (9) reported the synthesis of a Cys-tagged vector of VEGF_121_ by cloning two single-chain 3–112 amino acid fragments of VEGF_121_ joining head-to-tail to express as scVEGF in Escherichia coli for mammalian cell production. ^68^Ga labeling of scVEGF was performed through NOTA chelation (10). The NOTA group was activated by five-fold molar excess of N-hydroxysuccinimide-PEG-maleimide for 60 min (pH 8). A mixture of scVEGF and the activated NOTA in a molar ratio of 1:10 was incubated for 60 min. The NOTA-PEG-scVEGF conjugate was purified with high-performance liquid chromatography. The number of NOTA molecules per protein was ~1. For radiolabeling, 3 nmol NOTA-PEG-scVEGF was added to 30–50 MBq (0.81–1.35 mCi) ^68^Ga diluted in buffer (pH 4.2). ^68^Ga-NOTA-PEG-scVEGF was purified with column chromatography with a radiolabeling yield of 71%. ^68^Ga-NOTA-PEG-scVEGF was stable in phosphate-buffered saline (pH 7) for at least 4 h. Radiochemical purity and specific activity of the final preparation were not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=scVEGF+and+in+vitro)]

In vitro competition binding studies were performed in 293/KDR cells expressing cloned human VEGFR-2 (10). NOTA-PEG-scVEGF inhibited the binding of ^68^Ga-NOTA-PEG-scVEGF to VEGFR-2 on the cells with a K_d_ of 0.59 ± 0.20 nM and a B_max_ of 1.1 × 10^6^ binding sites per cell.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=scVEGF+rodentia)]

Eder et al. (10) performed ex vivo biodistribution studies of ^68^Ga-NOTA-PEG-scVEGF in nude mice (n = 3/group) bearing HT-29 human colon adenocarcinoma tumors expressing VEGFR-2 at 1, 2, 3, and 4 h after injection. The tumor accumulated 1.56%, 1.12%, 1.16%, and 1.06% injected dose per gram (ID/g) at 1, 2, 3, and 4 h, respectively. The blood concentration levels at these time points were 2.54%, 0.97%, 1.07%, and 0.52% ID/g, respectively. The organs with the highest accumulation of ^68^Ga-NOTA-PEG-scVEGF at 2 h after injection were the kidneys (119% ID/g), liver (5.3% ID/g), spleen (3.7% ID/g), and lung (3.5% ID/g). The tumor/blood and tumor/muscle ratios at 4 h after injection were 2.0 and 1.7, respectively. Injection of inactivated ^68^Ga-PEG-scVEGF showed only ~0.8% ID/g tumor accumulation at 1 h after injection. However, no blocking studies were performed. PET imaging studies were performed at 1.5 h after injection of ^68^Ga-NOTA-PEG-scVEGF with good tumor/background contrast.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=scVEGF+(dog+or+pig+or+sheep+or+rabbit))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=scVEGF+(primate+not+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=scVEGF+human)]

No publication is currently available.

## References

1 Ferrara N. (2004). Vascular endothelial growth factor: basic science and clinical progress. Endocr Rev.
2 Cohen T., Gitay-Goren H., Sharon R., Shibuya M., Halaban R., Levi B.Z., Neufeld G. (1995). VEGF121, a vascular endothelial growth factor (VEGF) isoform lacking heparin binding ability, requires cell-surface heparan sulfates for efficient binding to the VEGF receptors of human melanoma cells. J Biol Chem.
3 Itakura J., Ishiwata T., Shen B., Kornmann M., Korc M. (2000). Concomitant over-expression of vascular endothelial growth factor and its receptors in pancreatic cancer. Int J Cancer.
4 Ferrara N. (2004). Vascular endothelial growth factor as a target for anticancer therapy. Oncologist.
5 Hicklin D.J., Ellis L.M. (2005). Role of the vascular endothelial growth factor pathway in tumor growth and angiogenesis. J Clin Oncol.
6 Li S., Peck-Radosavljevic M., Koller E., Koller F., Kaserer K., Kreil A., Kapiotis S., Hamwi A., Weich H.A., Valent P., Angelberger P., Dudczak R., Virgolini I. (2001). Characterization of (123)I-vascular endothelial growth factor-binding sites expressed on human tumour cells: possible implication for tumour scintigraphy. Int J Cancer.
7 Li S., Peck-Radosavljevic M., Kienast O., Preitfellner J., Hamilton G., Kurtaran A., Pirich C., Angelberger P., Dudczak R. (2003). Imaging gastrointestinal tumours using vascular endothelial growth factor-165 (VEGF165) receptor scintigraphy. Ann Oncol.
8 Li S., Peck-Radosavljevic M., Kienast O., Preitfellner J., Havlik E., Schima W., Traub-Weidinger T., Graf S., Beheshti M., Schmid M., Angelberger P., Dudczak R. (2004). Iodine-123-vascular endothelial growth factor-165 (123I-VEGF165). Biodistribution, safety and radiation dosimetry in patients with pancreatic carcinoma. Q J Nucl Med Mol Imaging.
9 Backer M.V., Patel V., Jehning B.T., Claffey K.P., Backer J.M. (2006). Surface immobilization of active vascular endothelial growth factor via a cysteine-containing tag. Biomaterials.
10 Eder M., Krivoshein A.V., Backer M., Backer J.M., Haberkorn U., Eisenhut M. (2010). ScVEGF-PEG-HBED-CC and scVEGF-PEG-NOTA conjugates: comparison of easy-to-label recombinant proteins for [68Ga]PET imaging of VEGF receptors in angiogenic vasculature. Nucl Med Biol.